# Anti-mouse monoclonal antibody immunoglobulin G conjugated to GRKKRRQRRRPPQGYG-diethylenetriamine pentaacetic acid-[^111^In]

Chemical name: | Anti-mouse monoclonal antibody immunoglobulin G conjugated to GRKKRRQRRRPPQGYG-diethylenetriamine pentaacetic acid -[^111^In]
Abbreviated name: | [^111^In]mIgG-tat peptide
Synonym:
Agent Category: | Mouse immunoglobulin G
Target: | Cell nucleus
Target Category: | Nuclear uptake
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

Monoclonal antibodies (mAb) are often directed toward cell-surface molecules and may be radiolabeled for the imaging or treatment of cancer and other ailments (1-3). The radiolabeled mAbs are not readily internalized by the cell except by receptor-mediated endocytosis, which limits the use of these macromolecules either for the imaging or treatment of neoplastic solid tumors (4). However, Hu et al. showed that linking the mAb to the tat peptide (17 amino acid residues in the following sequence: GRKKRRQRRRPPQGYG) derived from the human immunodeficiency virus 1 (HIV-1) transactivator of the transcription (TAT) protein enabled it to be internalized and to be directed to the cellular nucleus (5, 6). Several investigators have used the tat peptide to enable cell penetration by a variety of large molecules including proteins, oligodeoxynucleotides, liposomes, and even nanoparticles (7-9). Conjugation of the tat peptide to mouse immunoglobulins (mIgG) labeled with radioactive iodine (^123^I) was shown to enhance cellular internalization of [^123^I]mIgG under in vitro conditions in human breast cancer MDA-MB-468 (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=HTB-132)cells and also in xenograft tumors derived from these cells in athymic mice (6). The investigators used a similar approach to construct and direct p21^WAF-1/Cip-1^, another ^123^I-labeled mAb against the intranuclear cyclin-dependent kinase inhibitor; p21^WAF-1/Cip-1^ was preferentially retained in xenograft tumors in athymic mice injected intratumorally with epidermal growth factor to induce the expression of p21^WAF-1/Cip-1^ (5). However, radiostability of the tat peptide (i.e., ^123^I-labeled mAb) is a major limitation of its use to target the intracellular or intranuclear epitopes because loss of the radiolabel can lead to the delivery of a suboptimal radioactivity dose to the cancerous lesions; in addition, ^123^I has a short half-life (13.3 h), so it is not possible to perform imaging studies for prolonged periods, especially when the tumor/background ratios are usually highest at 72 h after the administration of a radiolabeled mAb (10).

Press et al. showed that mAbs labeled with radioactive indium (^111^In; half-life = 2.8 days) and conjugated to the tat peptide were more stable in vivo compared with those labeled with ^123^I; ^111^In-labeled mAbs generate a higher tumor/background ratio, including internalization into the nucleus of human breast cancer BT-474 (http://www.biotech.ist.unige.it/cldb/cl498.html) cells (11). In addition, the ^111^In-labeled and tat peptide–conjugated, anti-mIgG ([^111^In]anti-mIgG-tat) were retained two times longer by the cells compared to the same tat peptide–linked mAb labeled with ^123^I (11). In an effort to extend this work, Cornelissen et al. investigated the biodistribution and nuclear importation of [^111^In]anti-mIgG-tat in normal tissue and BT-474 cell xenograft tumors in athymic mice (4). These studies are briefly described in this chapter.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+mIgG+tat+synthesis&WebEnv=0T0BGLDvTABh_BhGokCZQPnnHqQ90BFONl0wASn1-5MUjGdN-rzMH5yv2iAnsbI45VY-SpzH9A3ImI%407748428072881B60_0000SID&WebEnvRq=1)]

The synthesis of [^111^In]mIgG-tat was described by Cornelissen et al. (12). The tat peptide used for conjugation to the anti-mIgG was a synthetic peptide, but details of the chemistry used to prepare the peptide were not provided (12). Purity of the tat peptide was reported to be >97% as determined with high-performance liquid chromatography (HPLC).

Site-specific conjugation was used to link the [^111^In]tat to the anti-IgG mAb. The mIgG was obtained from commercial sources, and it was reacted with a four-fold molar excess of diethylenetriamine pentaacetic acid (DTPA) in anhydrous dimethyl sulfoxide. The reaction was allowed to proceed at room temperature for 45 min, and the DTPA-conjugated anti-mIgG was purified with size-exclusion HPLC (SE-HPLC) on a P-6 mini-column, with the use of phosphate-buffered saline (PBS) as the elution solvent. The anti-mIgG conjugate was determined to have 0.8 ± 0.3 mol DTPA/mol anti-mIgG. The purified DTPA-anti-mIgG was then mixed with an 800-fold molar excess of sodium periodide to generate aldehyde groups on the carbohydrates of the Fc domain of the mAb. After the oxidation reaction, a 40-fold molar excess of tat peptides (in PBS, pH 6.5) was added to the oxidized anti-mIgG, and the mixture was incubated in the dark at room temperature for 24 h. After this incubation, sodium cyanoborohydride (in PBS, pH 6.0) was added to the mixture to reduce the Schiff base between the tat peptide and the DTPA-anti-mIgG. The tat peptide–conjugated DTPA-anti-mIgG (anti-mIgG-tat) was then purified on a P-6 mini-column and eluted into citrate buffer (pH 5.0) (12). Under these conditions 1.2 ± 0.2 tat peptides were determined (n = 3 batches) to be substituted on each molecule of the anti-mIgG antibody.

Anti-mIgG-tat was labeled by exposing it to labeled indium (^111^In) chloride for 45 min at room temperature (12). The final radiochemical purity of the product was >95% as determined with instant thin-layer chromatography developed in sodium citrate buffer (pH 5.0); the Rf values for the various reaction components or the product were not provided. The specific activity of the labeled tat-anti-mIgG ([^111^In]anti-mIgG-tat) was 11,000 TBq/mmol (297.3 Ci/mmol).

The anti-mIgG conjugated to DTPA and modified with the tat peptide was reported to have the ability to recognize the same epitopes and to have a binding affinity that was similar to the unmodified parent mAb (12).

In another publication, the stability of [^111^In]anti-mIgG-tat was determined by incubating it in mouse plasma for 24–72 h, after which the amount of ^111^In associated with the anti-IgG or transferrin was determined with SE-HPLC (4). The labeled mAb was reported to be stable up to 24 h, but at 48 and 72 h, 2.9 ± 0.2% and 4.7 ± 0.3% of the label, respectively, was determined to be transchelated from [^111^In]anti-mIgG-tat to transferrin (n = 3 determinations). The investigators cautioned that, because the [^111^In]anti-mIgG-tat and transferrin peaks were not separated completely by SE-HPLC, the actual extent of transchelation could be higher than reported in the publication (4).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+mIgG+tat+in+vitro&WebEnv=03InJazHko8IxJrAkHXS3tK_1fApD9E_mru1SSevTYOidgaisz1yc6x24FrOulWyHUKzE_KWGkE7WQ%407748428072881B60_0000SID&WebEnvRq=1)]

Cornelissen et al. studied the cellular and nuclear penetration properties of [^111^In]anti-mIgG-tat with the use of BT-474 cells (12). The kinetics of [^111^In]anti-mIgG-tat uptake by the cells, cytoplasm, and nuclei was studied in the BT-474 cells. These investigators also performed competition studies with excess tat peptide or ammonium chloride (NH_4_Cl), an endosome acidification inhibitor(12). These results were compared with those obtained with ^111^In-labeled anti-IgG alone, which served as a control. The uptake and nuclear penetration of [^111^In]anti-mIgG-tat was reported to be two times greater compared with [^111^In]anti-mIgG, and the uptake was inhibited by the presence of either the tat peptide or NH_4_Cl. Of the total radioactivity taken up by the cells (127 ± 3.6 fmol) under these conditions, roughly half was detected in the cytoplasm (61.0 ± 2.5 fmol), and the other half was found in the nucleus (71.2 ± 3.0 fmol).

The efflux of incorporated radioactivity from the BT-474 cells after exposure to the labeled anti-mIgG was also studied (12). The cells were initially allowed to take up [^111^In]anti-mIgG-tat for 1 h at 37°C, and then the cells were washed and resuspended in growth medium for up to 24 h. During this time the amount of radioactivity remaining in the cell as free, cytoplasmic, and nuclear fractions was determined at various time points. The investigators reported that the elimination of radioactivity from the cell and the different compartments followed a biphasic model. Approximately 50% of the radioactivity was lost within 5 h, after which the amount of radioactivity remained constant within the cells, the cytoplasm and the nucleus (12).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

Cornelissen et al. investigated the biodistribution of [^111^In]anti-mIgG-tat in the tumors and normal tissue in athymic mice bearing subcutaneous BT-474 tumor xenografts (4). The uptake was compared after either an intravenous (IV) injection or intratumoral administration of [^111^In]anti-mIgG-tat (n = 3 animals) and compared with that of [^111^In]anti-mIgG (n = 3 animals) administered in the same manner. On the basis of the percent injected dose per gram tissue (% ID/g) and the area under the curve (AUC) calculations, after an IV injection of either radiochemical, [^111^In]anti-mIgG-tat (2.8 ± 0.2% ID/g) was reported to clear from blood two to three times faster than [^111^In]anti-mIgG (6.3 ± 1.5% ID/g) under these conditions at 72 h after injection (P = 0.0004). With the IV injection, at 72 h after administration, a two- to three-fold lower uptake of radioactivity was reported with [^111^In]anti-mIgG-tat compared to the control [^111^In]anti-mIgG, in the liver, lungs, and the small and large intestines of the animals (4). With either IV injected radiochemical, the accumulation of radioactivity was not significantly different in the kidneys or the xenograft tumors.

Cornelissen et al. also studied the uptake of [^111^In]anti-mIgG-tat and [^111^In]anti-mIgG in the normal and the tumor tissue after an intratumoral injection of the radiochemicals in the mice bearing a xenograft tumor (n = 3 animals/group and time point) (4). Uptake of radioactivity was determined at various time points up to 144 h after the intratumoral injection. The radioactivity was initially very high (146–154% ID/g) after an intratumoral injection that declined 12- to 14-fold by 144 h after administration. When administered intratumorally, the accumulation of [^111^In]anti-mIgG-tat in the tumors was higher than when it was administered intravenously to the animals. Also, the AUC was ~three-fold (610 ± 157% ID•h) for the intratumorally injected [^111^In]anti-mIgG-tat compared to an AUC of 200 ± 37% ID h for the intratumorally injected [^111^In]anti-mIgG. An intratumoral injection of [^111^In]anti-mIgG-tat resulted in an encased nuclear localization of radioactivity only in the tumor cell nuclei compared with an increased localization of the radioactivity in the nuclei of the tumor, liver, and kidneys after IV administration. Although the tumors were not imaged after an IV injection, the investigators reported that when they were imaged after an intratumoral injection, the radioactivity was located primarily in the tumors with both [^111^In]anti-mIgG-tat and [^111^In]anti-mIgG (4). From these results the investigators concluded that radiolabeled immunoconjugates of the tat peptide have a good potential use for imaging intracellular epitopes or for localized radiotherapy of tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+anti+mIgG+nonprimate+mammals&WebEnv=09AC2rOgYusw_AfEqMdlWWT2ZBWzNMDXq_LO4QgKqaysD1WnmFVxYqx6DQhuuoNgUu0jzDcmasExm3%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+anti+mIgG+nonhuman+primates&WebEnv=0ySUKBk-ZhTfqliEQIRFDhHUMCKpyQQQwX9R96mcxBicckt6rGrpM3-_OhZSGWsxOQknTfj3eUYzQC%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+anti+mIgG+human+studies&WebEnv=03MnadvTCz8b3-HONHHV_L_AHgsXkggumixDMVfH41O53MccVmkGPZ60_s35Igr7JFK00KQmvk3M6-%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Koyama Y., Barrett T., Hama Y., Ravizzini G., Choyke P.L., Kobayashi H. (2007). In vivo molecular imaging to diagnose and subtype tumors through receptor-targeted optically labeled monoclonal antibodies. Neoplasia.
2 Stillebroer A.B., Oosterwijk E., Oyen W.J., Mulders P.F., Boerman O.C. (2007). Radiolabeled antibodies in renal cell carcinoma. Cancer Imaging.
3 Dadachova E., Casadevall A. (2006). Treatment of infection with radiolabeled antibodies. Q J Nucl Med Mol Imaging.
4 Cornelissen B., McLarty K., Kersemans V., Scollard D.A., Reilly R.M. (2008). Properties of [(111)In]-labeled HIV-1 tat peptide radioimmunoconjugates in tumor-bearing mice following intravenous or intratumoral injection. Nucl Med Biol.
5 Hu M., Chen P., Wang J., Scollard D.A., Vallis K.A., Reilly R.M. (2007). 123I-labeled HIV-1 tat peptide radioimmunoconjugates are imported into the nucleus of human breast cancer cells and functionally interact in vitro and in vivo with the cyclin-dependent kinase inhibitor, p21(WAF-1/Cip-1). Eur J Nucl Med Mol Imaging.
6 Hu M., Chen P., Wang J., Chan C., Scollard D.A., Reilly R.M. (2006). Site-specific conjugation of HIV-1 tat peptides to IgG: a potential route to construct radioimmunoconjugates for targeting intracellular and nuclear epitopes in cancer. Eur J Nucl Med Mol Imaging.
7 Bullok K.E., Gammon S.T., Violini S., Prantner A.M., Villalobos V.M., Sharma V., Piwnica-Worms D. (2006). Permeation peptide conjugates for in vivo molecular imaging applications. Mol Imaging.
8 Torchilin V.P., Rammohan R., Weissig V., Levchenko T.S. (2001). TAT peptide on the surface of liposomes affords their efficient intracellular delivery even at low temperature and in the presence of metabolic inhibitors. Proc Natl Acad Sci U S A.
9 Zhang Y.M., Tung C.H., He J., Liu N., Yanachkov I., Liu G., Rusckowski M., Vanderheyden J.L. (2006). Construction of a novel chimera consisting of a chelator-containing Tat peptide conjugated to a morpholino antisense oligomer for technetium-99m labeling and accelerating cellular kinetics. Nucl Med Biol.
10 Reilly R.M., Sandhu J., Alvarez-Diez T.M., Gallinger S., Kirsh J., Stern H. (1995). Problems of delivery of monoclonal antibodies. Pharmaceutical and pharmacokinetic solutions. Clin Pharmacokinet.
11 Press O.W., Shan D., Howell-Clark J., Eary J., Appelbaum F.R., Matthews D., King D.J., Haines A.M., Hamann P., Hinman L., Shochat D., Bernstein I.D. (1996). Comparative metabolism and retention of iodine-125, yttrium-90, and indium-111 radioimmunoconjugates by cancer cells. Cancer Res.
12 Cornelissen B., Hu M., McLarty K., Costantini D., Reilly R.M. (2007). Cellular penetration and nuclear importation properties of 111In-labeled and 123I-labeled HIV-1 tat peptide immunoconjugates in BT-474 human breast cancer cells. Nucl Med Biol.